# 2-Butyl-5-[^11^C]methoxymethyl-6-(1-oxopyridin-2-yl)-3-[[2'-(1H-tetrazol-5-yl)biphenyl-4-yl]methyl]-3H-imidazo[4,5-b]pyridine

Chemical name: | 2-Butyl-5-[^11^C]methoxymethyl-6-(1-oxopyridin-2-yl)-3-[[2'-(1H-tetrazol-5-yl)biphenyl-4-yl]methyl]-3H-imidazo[4,5-b]pyridine
Abbreviated name:
Synonym: | [^11^C]KR31173
Agent category: | Compound
Target: | Angiotensin type 1 (AT_1_) receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-Human Primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173)]

Angiotensin II (Ang II), an octapeptide, plays an important role in the regulation of cardiovascular, renal and endocrine function (1, 2). Ang II induces a variety of physiological changes such as constricting of vascular smooth muscle cells, modulation of glomerular filtration rate, and sodium retention, resulting in an increase in blood pressure. Two subtypes of Ang II receptors, AT_1_ and AT_2_, have been well characterized pharmacologically and biochemically (3, 4). AT_1_ is indicated in all known pressor effects of Ang II, whereas no known biological functions have been found for AT_2_. The AT_1_ receptor subtype is found mainly in all vascular tissues, the pituitary gland and is the only subtype in the liver. The AT_2_ receptor subtype is found mainly in the rat adrenal medulla, human uterus, rat ovarian granulosa cells, and rat striatum. In other tissues, such as the adrenal cortex, kidneys, heart and brain, there is a mixture of both subtypes.

The AT_1_ nonpeptide antagonist, losartan (MK-954 or DuP753), was shown to be effective anti-hypertensive agent (5). MK-996 (L-159,282) was found to be a potent and selective AT_1_ antagonist with high affinity (IC_50_ = 0.15 nM for AT_1_ and >300 nM for AT_2_) (6). L159,884, the methoxyl analog of MK-996 (IC_50_, 0.08 nM), has been radiolabeled as [^11^C]L-159,884 for in vivo investigation of AT_1_ expression by PET in the kidneys, adrenal gland and heart (7). Another nonpeptide AT_1_ antagonist (IC_50_, 3.27 nM), 2-Butyl-5-methoxymethyl-6-(1-oxopyridin-2-yl)-3-[[2'-(1H-tetrazol-5-yl)biphenyl-4-yl]methyl]-3H-imidazo[4,5-b]pyridine (KR31173), is a methoxyl analog of SK-1080, which has been shown to be a selective AT_1_ antagonist (IC_50_, 11.6 nM) (8). [^11^C]KR31173 (2-Butyl-5-[^11^C]methoxymethyl-6-(1-oxopyridin-2-yl)-3-[[2'-(1H-tetrazol-5-yl)biphenyl-4-yl]methyl]-3H-imidazo[4,5-b]pyridine) is being studied as a radioligand for PET imaging of AT_1_ receptors.

### Related Resource Links

- Chapters in MICAD (AT_1_ (http://www.ncbi.nlm.nih.gov/books?term=AT1%20receptor%20%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (AT_1_ (http://www.ncbi.nlm.nih.gov/gene/185)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (AT_1_ (http://omim.org/entry/106165))
- Clinical trials (AT_1_ (http://www.clinicaltrials.gov/ct2/results?term=Angiotensin+II+receptor))
- Drug information in FDA (AT_1_ (http://google-test.fda.gov/search?q=Angiotensin+II+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173%20and%20synthesis)]

Mathews et al. (9) reported synthesis of [^11^C]KR31173 by O-methylation of the corresponding desmethyl phenolic precursor with [^11^C]methyl chloride in the presence of NaH in DMF or terahydrofuran, followed by acid hydrolysis to remove the protecting group from the tetrazole moiety. An average radiochemical yield was 5% (based on [^11^C]methyl chloride, not corrected for decay) with a total synthesis time of 25 min. An average specific activity was 258.3 GBq/μmol (6979 mCi/μmol at end of synthesis) with a radiochemical purities of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173%20and%20in%20vitro)]

KR31173 was shown to have an IC_50_ of 3.27 nM determined using rat liver homogenates (AT_1_) (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173%20and%20rodentia)]

Biodistribution studies in mice were performed by Mathews et al. (9) showing high accumulation of radioactivity in the liver (30.32% injected dose (ID)/g), followed by the kidney (22.70% ID/g), adrenal (19.71% ID/g), lung (3.23% ID/g), and heart (2.16% ID/g) at 5 min after injection of [^11^C]KR31173. There was marked accumulation of the tracer in the liver within the first 5 min, followed by a rapid decrease of radioactivity to 4.56% ID/g at 90 min. After 30 min, the highest accumulation was in the adrenal gland and kidney with tissue/blood ratios >10. Pretreatment (1-2 mg/kg) with MK-996, KR31173 or SK-1080 effectively inhibited specific binding of [^11^C]KR31173 to the adrenal glands (91-98% inhibition), kidneys (82-90%), lungs (88-96%) and heart (92-96%) (9, 10). Only 33-50% inhibition was seen in the liver. PET imaging of mice showed that renal accumulation of radioactivity was inhibited by 49 ± 6% at 10-60 min with SK-1080 pretreatment (10).

Higuchi et al. (11) performed [^11^C]KR31173 PET imaging studies in a myocardial ischemia reperfusion injury rat model. The left coronary artery was ligated for 20-25 min with subsequent perfusion for 16–18 h. A 30-min static scan was obtained at 20 min after the intravenous injection of 55.5 MBq (1.5 mCi) of [^11^C]KR31173 at 7 d after the induction of ischemia (n = 3). The infarct/normal ratio was 2.2 ± 0.9. The ratio decreased to 1.26 ± 0.10 (P < 0.01) with SK-1080 pretreatment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

Zober et al. (10) performed PET imaging quantitative measurements of [^11^C]KR31173 binding in the kidneys of three dogs with kinetic and graphical analyses (Logan), using arterial input function. The dogs were injected intravenously with 275 ± 58 MBq (7.43 ± 1.57 mCi) of [^11^C]KR31173. PET scans showed distinct accumulation of [^11^C]KR31173 in the adrenal and renal cortex. Renal accumulation and kinetics of [^11^C]KR31173 were imaged at baseline and after pretreatment with 1 mg/kg AT_1_ antagonist SK-1080. Within the time interval between 75 and 95 min after injection, the radioactivity retained in the kidneys was 63 nCi/ml/mCi of the injected dose for the control and was reduced by 92% with SK-1080 pretreatment, The distribution volume of [^11^C]KR31173 decreased by 84% from a baseline of 5.71 ± 0.56 to a post-SK-1080 value of 0.90 ± 0.13.These results demonstrate distinct binding of [^11^C]KR31173 in the renal cortex with a specific binding component suitable for quantitative PET imaging of AT_1_ receptors. The fraction of unchanged [^11^C]KR31173 in plasma samples determined by HPLC was 15% at 90 min after injection.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173%20and%20(primate%20not%20human))]

Zober et al. (10) studied one male baboon with [^11^C]KR31173 and [^11^C]L-159884 PET imaging under baseline conditions and after pretreatment with SK-1080. There was a higher accumulation of [^11^C]KR31173 (345 nCi/ml/mCi injected dose) than [^11^C]L-159884 (96 nCi/ml/mCi injected dose) in the renal cortex. Pretreatment with SK-1080 revealed that the specific binding of [^11^C]KR31173 was higher (81%) than the specific binding of [^11^C]L-159,884 (34%). The distribution volume (Logan analysis) of [^11^C]KR31173 decreased by 92% from a baseline of 13 to a post-SK-1080 value of 1. On the other hand, The distribution volume of [^11^C]L-159,884 decreased only by 12% from a baseline of 1.5 with SK-1080 pretreatment. The fraction of unchanged [^11^C]KR31173 in plasma samples determined by HPLC was 21% at 90 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KR31173%20and%20human)]

No publication is currently available.

## NIH Support

1RO1 HL092985, 5RO1 DK050183, 5U24 CA092871-10

## References

1 Ferrario C.M. (1990). The renin-angiotensin system: importance in physiology and pathology. J Cardiovasc Pharmacol.
2 Griendling K.K., Murphy T.J., Alexander R.W. (1993). Molecular biology of the renin-angiotensin system. Circulation.
3 Griendling K.K., Lassegue B., Murphy T.J., Alexander R.W. (1994). Angiotensin II receptor pharmacology. Adv Pharmacol.
4 Timmermans P.B., Chiu A.T., Herblin W.F., Wong P.C., Smith R.D. (1992). Angiotensin II receptor subtypes. Am J Hypertens.
5 Duncia J.V., Carini D.J., Chiu A.T., Johnson A.L., Price W.A., Wong P.C., Wexler R.R., Timmermans P.B. (1992). The discovery of DuP 753, a potent, orally active nonpeptide angiotensin II receptor antagonist. Med Res Rev.
6 Chakravarty P.K., Naylor E.M., Chen A., Chang R.S., Chen T.B., Faust K.A., Lotti V.J., Kivlighn S.D., Gable R.A., Zingaro G.J., et al. (1994). A highly potent, orally active imidazo[4,5-b]pyridine biphenylacylsulfonamide (MK-996; L-159,282): a new AT1-selective angiotensin II receptor antagonist. J Med Chem.
7 Hamill T.G., Burns H.D., Dannals R.F., Mathews W.B., Musachio J.L., Ravert H.T., Naylor E.M. (1996). Development of [11C]L-159,884: a radiolabelled, nonpeptide angiotensin II antagonist that is useful for angiotensin II, AT1 receptor imaging. Appl Radiat Isot.
8 Lee S.H., Jung Y.S., Lee B.H., Yun S.I., Yoo S.E., Shin H.S. (1999). Characterization of angiotensin II antagonism displayed by SK-1080, a novel nonpeptide AT1-receptor antagonist. J Cardiovasc Pharmacol.
9 Mathews W.B., Yoo S.E., Lee S.H., Scheffel U., Rauseo P.A., Zober T.G., Gocco G., Sandberg K., Ravert H.T., Dannals R.F., Szabo Z. (2004). A novel radioligand for imaging the AT1 angiotensin receptor with PET. Nucl Med Biol.
10 Zober T.G., Mathews W.B., Seckin E., Yoo S.E., Hilton J., Xia J., Sandberg K., Ravert H.T., Dannals R.F., Szabo Z. (2006). PET Imaging of the AT1 receptor with [11C]KR31173. Nucl Med Biol.
11 Higuchi T., Fukushima K., Xia J., Mathews W.B., Lautamaki R., Bravo P.E., Javadi M.S., Dannals R.F., Szabo Z., Bengel F.M. (2010). Radionuclide imaging of angiotensin II type 1 receptor upregulation after myocardial ischemia-reperfusion injury. J Nucl Med.